# ^177^Lu-DOTA-Tyr^3^-c(Cys-Tyr-Trp-Lys-Thr-Cys)-Thr-Lys(cypate)-NH_2_

Chemical name: | ^177^Lu-DOTA-Tyr^3^-c(Cys-Tyr-Trp-Lys-Thr-Cys)-Thr-Lys(cypate)-NH_2_
Abbreviated name: | ^177^Lu-LS172
Synonym: | ^177^Lu-DOTA-Tyr^3^-octreotate-Lys-cypate, ^177^Lu-DOTA-Y3-TATE-Lys-cypate
Agent category: | Peptide
Target: | Somatostatin receptor subtype-2 (SSTR-2)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), near-infrared (NIR) fluorescent imaging, optical fluorescent imaging
Source of signal/contrast: | ^177^Lu, cypate
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=177Lu + LS172)]

Somatostatin (SST) (somatotropin release-inhibiting hormone, somatotropin release-inhibiting factor) is a cyclic disulphide-containing peptide hormone of 14 amino acids (1). SST inhibits hormone secretion, cell proliferation, and promotes apoptosis through binding to specific cell-surface somatostatin receptors (SSTRs) (2). Five SSTR subtypes are identified in the central nervous system (CNS), gastrointestinal tract, and a variety of benign and malignant tumors (2). All subtypes of SSTRs belong to the family of G protein–coupled receptors, and exhibit high affinity to SST by recognizing the β-turn in the peptide sequence of SST including Phe7, Trp8, Lys9, and Thr10 (2). The structural difference between SSTRs generates specific pharmacological and physiological properties for each subtype, which allows targeting of SSTRs with subtype-specific SST analogs (1). For example, octreotide, a SST analog with a peptide sequence of eight amino acids (D-Phe-c(Cys-Tyr-D-Trp-Lys-Thr-Cys)-Thr(ol)), possesses a much higher affinity (~2 nM) binding to SSTR-2, -3, and -5 than binding to SSTR-1 and -4 (>1,000 nM). In addition to symptomatic treatment of tumors in clinic, these analogs are also labeled with a variety of probes for imaging (1).

^177^Lu-DOTA-Tyr^3^-c(Cys-Tyr-Trp-Lys-Thr-Cys)-Thr-Lys(cypate)-NH_2_(^177^Lu-LS172) is a monomolecular multimodal imaging agent (MOMIA) for single-photon emission computed tomography (SPECT) and optical imaging (3). ^177^Lu-LS172 consists of three components: a STT analog Tyr3-octreotate (Y3-TATE) with an additional lysine at the N-terminal as a spacer linker, a complex of ^177^Lu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (^177^Lu-DOTA) attached at the C-terminal of Y3-TATE, and a cypate attached at the ε-amine group of the spacer lysine at the N-terminal of Y3-TATE. As a STT analog, TATE is produced by replacing the C-terminal threoninol in the octreotide with threonine, which substantially increases the binding affinity for SSTR-2 (1). ^177^Lu is a radionuclide belonging to the group of rare earth isotopes, and it is produced by neutron bombardment of purified target materials in reactors (4). With a half-life of 6.71 days for β^-^ emission at 498 keV and 78% branch fraction, ^177^Lu has been a very promising radionuclide in radiotherapy for effectively destroying small tumors and metastasis (optimal size 1.2–3.0 mm) while sparing normal tissue (5). ^177^Lu also emits low energetic gamma rays at 208 and 113 keV with 10% and 6% abundance, respectively, which allows for direct monitoring of the activity distribution by SPECT and subsequent dosimetry (5). ^177^Lu-DOTA-Y3-TATE has demonstrated excellent tumor localization, good clearance properties, and significant tumor regression in animal models (6). Cypate (mw 625.34) is a carbocyanine derivative with structure and optical properties very similar to indocyanine green dye (ICG). Cypate exhibits a high extinction coefficient (224,000 M^-1^cm^-1^) in the near-infrared (NIR) region (700–900 nm) (3, 7). The low light scattering and absorption of endogenous photoactive biomolecules in this region permit photons to penetrate several centimeters into tissues (8, 9). Two carboxyl groups in cypate can be conjugated with amines to generate peptide-based optical imaging agents (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu + LS172)+AND+synthesis%0D%0A)]

The synthesis of ^177^Lu-LS172 was conducted in several steps (3). Y3-TATE was synthesized with a peptide synthesizer by standard automated Fmoc protocols. Rink amide resin was initially loaded with Fmoc amino acids followed by automatic activation of the carboxyl group with a mixture of 1-hydroxybenzotriazole (HOBt) and o-(benzotriazol-1-yl)-N,N,N',N'-tetramethyluronium hexafluorophosphate (HBTU) and subsequent coupling with Fmoc-protected amino acid. LS172 was produced by attaching DOTA and cypate to Y3-TATE in situ. The carboxylic acid of tri-t-butyl-DOTA was coupled to the amine of the N-terminal phenylalanine, and the carboxylic acid of cypate was coupled to the ε-amino group of the C-terminal lysine. The overall yield of LS172 was found to be 96%. The radiolabling of LS172 was accomplished by mixing ^177^LuCl_3_ (100 μCi) with LS172 in a buffer (pH 4.0) and incubated at 80ºC for 80 min. The produced ^177^Lu-LS172 had a radiochemical purity of ≥99% and a final specific activity of 12.5 Ci/g (27 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu + LS172)+AND+%22in+vitro%22)]

The spectral and binding properties of LS172 were examined in vitro (3). Similar to cypate, LS172 exhibited broad excitation and emission bands with a narrow Stokes shift (23 nm). The relative quantum yield of LS172 (0.12) was the same as that of ICG. Because of the modifications in both C- and N-terminal, the affinity of LS172 binding to SSTR-2 increased ~10- and ~5-fold relative to cypate-Y3-TATE and Y3-TATE, respectively. The complexation with Lu^3+^ appeared not to affect the resultant affinity (2.14 nM for Lu-LS172 versus 2.03 nM for LS172). The internalization of LS172 was evaluated with NIR fluorescence microscopy in A427-7 membranes (SSTR-2–positive) and HEK293 cells (STTR-2–negative). LS172 was weakly internalized at 25 nM. The internalization was inhibited by 5 μM Y3-TATE with an incubation time <60 min. In comparison, cypate-Y3-TATE was strongly internalized in a time-dependent manner, and the internalization was completely blocked by 5 μM Y3-TATE.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu + LS172) +AND++rodentia)]

The biochemical distribution of LS172 was examined in AR42J tumors in rats (n = 5) (3). ^177^Lu-LS172 (6.2 Ci/230 mmol (500 mg/230 mmol)) was injected intravenously in rats at 10–14 days after tumor implantation in the legs or after the tumors had grown ~1.5–2.0 g. In another group of tumor-implanted rats (n = 5), Y3-TATE (100μg/95 nmol) was also included as a competitive dose in addition to the radiolabeled LS172. The pharmacokinetic profile ^177^Lu-LS172 exhibited a rapid blood clearance of 0.228 ± 0.047% injected dose per gram (ID/g) (0.151 ± 0.027% ID/g) at 1 h after injection. Clearance of ^177^Lu-LS172 was predominately hepatic (17.862 ± 3.286% ID/g, 89.6 ± 3.16% ID/liver, 1 h) with relatively low kidney accumulation (1–2%). Accumulation of activity for ^177^Lu-LS172 in the SSTR-2–positive tissues of adrenal, pituitary, pancreas, and tumor were relatively low (≤1% ID/g). With a co-administration of Y3-TATE, the accumulation of ^177^Lu-LS172 decreased significantly in all SSTR-2–positive tissue except the bone.

The NIR fluorescence imaging of LS172 was performed in tumor-bearing NCR nu/nu mice (n = 6) (3). After inoculation with lung adenocarcinoma cell line A427-7 in the right and left flanks of each mouse, tumors were allowed to grow to 5–10 mm maximum diameter before imaging. Three mice were injected with 2 nmol LS172, and two other mice were injected with 2 nmol LS172 and a competitive dose of 95 nmol Y3-TATE. NIR fluorescence images were collected at 1, 4, 8, and 24 h after injection. No significant accumulation of LS172 was found in tumors compared to that in normal tissue at different time points. The competitive inhibition with Y3-TATE did not significantly alter the tumor/muscle uptake ratio. After 24 h, the mice were euthanized, and tissues were harvested for ex vivo fluorescence biodistribution imaging. In addition to the liver and kidneys, LS172 accumulated in the spleen and accounted for 35% of the fluorescence intensity relative to that in the liver. LS172 accumulation in mouse kidney was somewhat higher than that of the radiolabeled analogs in rat kidneys, possibly indicating the reduction of overall charge on the DOTA upon chelation with a metal ion. The uptake and clearance profiles of LS172 in tumor-bearing A427-7 mice were similar to those of ^177^Lu-LS172 in tumor-bearing AR427 rats.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu + LS172) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu + LS172) +AND+human)]

No publication is currently available.

### NIH Support

CA 100972, EB 1430, CA 123537, CA 64475

## References

1 Breeman W.A., Kwekkeboom D.J., de Blois E., de Jong M., Visser T.J., Krenning E.P. (2007). Radiolabelled regulatory peptides for imaging and therapy. Anticancer Agents Med Chem.
2 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
3 Edwards W.B., Xu B., Akers W., Cheney P.P., Liang K., Rogers B.E., Anderson C.J., Achilefu S. (2008). Agonist-antagonist dilemma in molecular imaging: evaluation of a monomolecular multimodal imaging agent for the somatostatin receptor. Bioconjug Chem.
4 Schotzig U., Schrader H., Schonfeld E., Gunther E., Klein R. (2001). Standardisation and decay data of 177Lu and 188Re. Appl Radiat Isot.
5 Dvorakova Z., Henkelmann R., Lin X., Turler A., Gerstenberg H. (2008). Production of 177Lu at the new research reactor FRM-II: Irradiation yield of 176Lu(n,gamma)177Lu. Appl Radiat Isot.
6 de Jong M., Breeman W.A., Bernard B.F., Bakker W.H., Schaar M., van Gameren A., Bugaj J.E., Erion J., Schmidt M., Srinivasan A., Krenning E.P. (2001). [177Lu-DOTA(0),Tyr3] octreotate for somatostatin receptor-targeted radionuclide therapy. Int J Cancer.
7 Achilefu S., Dorshow R.B., Bugaj J.E., Rajagopalan R. (2000). Novel receptor-targeted fluorescent contrast agents for in vivo tumor imaging. Invest Radiol.
8 Mahmood U., Weissleder R. (2003). Near-infrared optical imaging of proteases in cancer. Mol Cancer Ther.
9 Ye Y., Bloch S., Xu B., Achilefu S. (2008). Novel near-infrared fluorescent integrin-targeted DFO analogue. Bioconjug Chem.
10 Zhang Z., Achilefu S. (2005). Spectral properties of pro-multimodal imaging agents derived from a NIR dye and a metal chelator. Photochem Photobiol.